# ^99m^Tc-(Hydrazinonicotinic acid-β-Ala-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_)(tricine)(TPPTS)

Chemical name: | ^99m^Tc-(Hydrazinonicotinic acid-β-Ala-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH2)(tricine)(TPPTS)
Abbreviated name: | ^99m^Tc-HYNIC-ABN, ^99m^Tc-(HYNIC-ABN)(tricine)(TPPTS)
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | SPECT, gamma planar imaging
Source of signal\contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+ABN+)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids), is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of 7 amino acids, -Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on CNS and GI tissues and a number of tumor cell lines (4). The BBN-R superfamily includes at least 4 different subtypes, namely neuromedin B (NMB or BB1), the GRPR subtype (BB2), BB3, and BB4. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Shi et al. (7) have used a ternary ligand system (HYNIC, tricine and TPPTS) for labeling β-Ala-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (ABN). HYNIC (hydrazinonicotinic acid) is a bifunctional coupling agent for ^99m^Tc-labeling, while tricine and TPPTS (trisodium triphenylphosphine-3,3',3''-trisulfonate) were used as coligands to prepare the ternary ligand complex [^99m^Tc(HYNIC-ABN)(tricine)(TPPTS)] for SPECT imaging GRPR of colon cancer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+ABN+synthesis)]

A solution (0.32 ml) of tricine (10 mg), SnCl_2_ (0.06 mg), 370 MBq (10 mCi) Na^99m^TcO_4_ and HYNIC-ABN (0.01 mg) was incubated at room temperature for 10 min (7). A solution (0.1 ml) of TPPTS (6 mg) was added in the reaction mixture and heated at 100°C for 30 min. ^99m^Tc(HYNIC-ABN)(tricine)(TPPTS) was purified with Sep-Pak. The specific activity of the purified product was 44.4 GBq/mmol (1.2 Ci/mmol) with a radiochemical purity of >95%. The logP value was -2.39. ^99m^Tc(HYNIC-ABN)(tricine)(TPPTS) was >95% intact after 12 h in saline and in the presence of 1 mg/ml of cysteine.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+ABN+in+vitro)]

Shi et al. (7) performed in vitro inhibition studies of ABN and HYNIC-ABN in cultured PC-3 human prostate cancer cells with ^125^I-[Tyr4]BBN. The IC_50_ values were 24 ± 2 nM and 38 ± 1 nM, respectively. In vitro internalization and efflux studies of ^99m^Tc(HYNIC-ABN)(tricine)(TPPTS) were performed in cultured HT-29 human colon cancer cells at 37ºC. HT-29 cells exhibited a rapid internalization with 35% of radioactivity at 5 min after incubation and reached a maximal cellular radioactivity of 68% at 30 min. However, only ~20% of the internalized radioactivity remained after 1 h of incubation in tracer-free medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+ABN+%20rodentia)]

Shi et al. (7) performed biodistribution studies of ^99m^Tc(HYNIC-ABN)(tricine)(TPPTS) in nude mice bearing HT-29 xenografts. Tumor uptake values were 1.59% ID/g at 30 min, 1.2% ID/g at 60 min, and 0.8% ID/g at 120 min. The organ with the highest uptake was the kidney (~9% ID/g) with little radioactivity in the muscle (0.14% ID/g), blood (0.50% ID/g), intestine (0.63% ID/g), lung (0.60% ID/g) and liver (0.68% ID/g) at 60 min after injection. Tumor/blood, tumor/liver, and tumor/muscle ratios were 2.37, 1.69, and 11.17, respectively. Most of the injected radioactivity was found in the urine sample at 60 min after injection. No intact ^99m^Tc(HYNIC-ABN)(tricine)(TPPTS) was detected in the urine, kidney, and liver samples at 60 min after injection. SPECT imaging in nude mice bearing HT-29 xenografts was performed with 14.8 MBq (0.4 mCi) of ^99m^Tc(HYNIC-ABN)(tricine)(TPPTS). The tumors, kidneys and urinary bladder were clearly visualized at 1 h after injection. Pre-administration of excess HYNIC-ABN substantially inhibited the radioactivity in the tumors, liver, stomach, intestine and kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+ABN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+ABN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+ABN+human)]

No publication is currently available.

## NIH Support

R01 CA115883

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Shi J., Jia B., Liu Z., Yang Z., Yu Z., Chen K., Chen X., Liu S., Wang F. (2008). 99mTc-labeled bombesin(7-14)NH2 with favorable properties for SPECT imaging of colon cancer. Bioconjug Chem.